# ^111^In-1,4,7,10-Tetraazacyclododecane-1,4,7,10-triacetic acid-8-aminooctanoic acid-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_

Chemical name: | ^111^In-1,4,7,10-Tetraazacyclododecane-1,4,7,10-triacetic acid-8-aminooctanoic acid-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_
Abbreviated name: | ^111^In-DOTA-8-Aoc-BBN[7-14]NH_2_
Synonym:
Agent category: | Peptide
Target: | Gastrin-releasing peptide receptor (GRPR)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar
Source of signal\contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=4885361), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=61677286) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2925) for more information about gastrin-releasing peptide receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+DOTA+111In)]

The amphibian bombesin (BBN or BN, a peptide of 14 amino acids) is an analog of human gastrin-releasing peptide (GRP, a peptide of 27 amino acids) that binds to GRP receptors (GRPR) with high affinity and specificity (1, 2). Both GRP and BBN share an amidated C-terminus sequence homology of seven amino acids, Trp-Ala-Val-Gly-His-Leu-Met-NH_2_. BBN-Like peptides have been shown to induce various biological responses in diverse tissues, including the central nervous system and the gastrointestinal system. They also act as potential growth factors for both normal and neoplastic tissues (3). Specific BBN receptors (BBN-R) have been identified on central nervous system and gastrointestinal tissues and on a number of tumor cell lines (4). The BBN-R superfamily includes at least four different subtypes, namely the GRPR subtype (BB2), the neuromedin B (NMB) receptor subtype (BB1), the BB3 subtype, and the BB4 subtype. The findings of GRPR overexpression in various human tumors, such as breast, prostate, lung, colon, ovarian, and pancreatic cancers, provide opportunities for tumor imaging by designing specific molecular imaging agents to target the GRPR (5, 6).

Various BBN analogs have been labeled with ^99m^Tc and ^111^In for single-photon emission computed tomography (SPECT) imaging studies (7) and with ^64^Cu, ^68^Ga, and ^86^Y for positron emission tomography imaging studies (8, 9). Hoffman et al. (10) used 1,4,7,10-tetraazacyclododecane-1,4,7,10-triacetic acid (DOTA) as a bifunctional chelator for labeling 8-aminooctanoic acid-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_ (8-Aoc-BBN[7-14]NH_2_) with ^111^In (t_1/2_, 2.8 d). ^111^In-DOTA-8-Aoc-BBN[7-14]NH_2_ has been evaluated as a SPECT imaging agent of GRPR in nude mice bearing human PC-3 prostate cancer cells.

### Related Resource Links:

- Chapters in MICAD (GRPR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=(GRPR%20OR%20GRP-R)%20+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad), bombesin (http://www.ncbi.nlm.nih.gov/books?term=bombesin%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (GRPR (http://www.ncbi.nlm.nih.gov/gene/2925), GRP (http://www.ncbi.nlm.nih.gov/gene/2922))
- Articles in Online Mendelian Inheritance in Man (OMIM) (GRPR (http://www.ncbi.nlm.nih.gov/omim/305670), GRP (http://omim.org/entry/137260))
- Clinical trials (GRPR (http://www.clinicaltrials.gov/ct2/results?term=bombesin))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+DOTA+111In+synthesis)]

DOTA-8-Aoc-BBN[7-14]NH_2_ was prepared with solid-phase peptide synthesis (10). ^111^InCl_3_ (37 MBq, 1 mCi) was added to a solution of DOTA-8-Aoc-BBN[7-14]NH_2_ (68 nmol) in tetramethylammonium acetate buffer (pH 5.8). The mixture was heated for 60 min at 80°C. The product, ^111^In-DOTA-8-Aoc-BBN[7-14]NH_2_, was purified with high-performance liquid chromatography, with a radiochemical yield of 75%–80% after purification and a radiochemical purity of >99%. The specific activity of ^111^In-DOTA-8-Aoc-BBN[7-14]NH_2_ was not reported. ^111^In-DOTA-8-Aoc-BBN[7-14]NH_2_ remained 50% intact in human serum after 17.3 h of incubation.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+DOTA+111In+in+vitro)]

Hoffman et al. (10) performed in vitro inhibition studies of ^nat^In-DOTA-8-Aoc-BBN[7-14]NH_2_ in cultured human prostate PC-3 tumor cells with ^125^I-Tyr^4^-BBN. The 50% inhibition concentration (IC_50_) value was 0.6 ± 0.1 nM. ^nat^In-DOTA-BBN[7-14]NH_2_ exhibited the IC_50_ value of 110.6 ± 32.3 nM. The addition of 8-Aoc improved the affinity of ^nat^In-DOTA-8-Aoc-BBN[7-14]NH_2_ over ^nat^In-DOTA-BBN[7-14]NH_2._ PC-3 cells exhibited rapid internalization of ^111^In-DOTA-8-Aoc-BBN[7-14]NH_2_, with >70% of radioactivity inside the cells at 60 min of incubation.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+DOTA+111In%20rodentia)]

Ex vivo biodistribution studies of 2.8 MBq (0.075 mCi) ^111^In-DOTA-8-Aoc-BBN[7-14]NH_2_ were performed in nude mice (n = 5/group) bearing PC-3 xenografts at 0.25, 0.5, 1, 4, and 24 h (10). Tumor accumulation at these time points was 7.59 ± 2.11, 4.58 ± 0.53, 3.63 ± 1.11, 1.78 ± 1.09, and 1.56 ± 0.45% injected dose per gram (ID/g), respectively. The organ with the highest accumulation was the pancreas (18.8% ID/g), followed by the small intestine (6.80% ID/g), kidney (5.66% ID/g), large intestine (4.29% ID/g), stomach (1.99% ID/g), spleen (1.39% ID/g), and liver (1.34% ID/g) at 1 h after injection. The urinary excretion was 68% ID at 1 h. Blood concentration was 0.6% ID/g at 1 h and 0.1% ID/g at 24 h. Co-injection with excess BBN[1-14] (100 µg/mouse) inhibited the tumor accumulation by 65% at 1 h after tracer injection. Accumulation levels in the pancreas, stomach, spleen, large intestine, and small intestine were inhibited by 98%, 83%, 85%, 95%, and 68%, respectively. Little inhibition was observed in the blood (0.68% ID/g). No SPECT imaging studies were performed.

Winkelmann et al. (11) performed SPECT imaging studies in immunocompromised nude mice (n = 17) with PC-3 bone metastases (intracardiac injection of PC-3 tumor cells) after injection of 7.4 MBq (0.2 mCi) ^111^In-DOTA-8-Aoc-BBN[7-14]NH_2._ Mice (n = 13) with bone lesions (confirmed with computed tomography imaging; n = 4/mouse) were used in the studies. ^111^In-DOTA-8-Aoc-BBN[7-14]NH_2_ SPECT imaging successfully identified small, osteolytic bone lesions that correlated the areas of increased radioactivity with CT images. The bone lesions were confirmed with histopathology.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+DOTA+111In%20and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+DOTA+111In+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+DOTA+111In+human)]

No publication is currently available.

## NIH Support

1P20 CA72942, RO1 CA72942

## References

1 Gonzalez N., Moody T.W., Igarashi H., Ito T., Jensen R.T. (2008). Bombesin-related peptides and their receptors: recent advances in their role in physiology and disease states. Curr Opin Endocrinol Diabetes Obes.
2 Bertaccini G. (1976). Active polypeptides of nonmammalian origin. Pharmacol Rev.
3 Chung D.H., Evers B.M., Beauchamp R.D., Upp J.R., Rajaraman S., Townsend C.M., Thompson J.C. (1992). Bombesin stimulates growth of human gastrinoma. Surgery.
4 Benya R.V., Kusui T., Pradhan T.K., Battey J.F., Jensen R.T. (1995). Expression and characterization of cloned human bombesin receptors. Mol Pharmacol.
5 Reubi J.C., Wenger S., Schmuckli-Maurer J., Schaer J.C., Gugger M. (2002). Bombesin receptor subtypes in human cancers: detection with the universal radioligand (125)I-[D-TYR(6), beta-ALA(11), PHE(13), NLE(14)] bombesin(6-14). Clin Cancer Res.
6 Smith C.J., Volkert W.A., Hoffman T.J. (2005). Radiolabeled peptide conjugates for targeting of the bombesin receptor superfamily subtypes. Nucl Med Biol.
7 Varvarigou A., Bouziotis P., Zikos C., Scopinaro F., De Vincentis G. (2004). Gastrin-releasing peptide (GRP) analogues for cancer imaging. Cancer Biother Radiopharm.
8 Biddlecombe G.B., Rogers B.E., de Visser M., Parry J.J., de Jong M., Erion J.L., Lewis J.S. (2007). Molecular imaging of gastrin-releasing peptide receptor-positive tumors in mice using 64Cu- and 86Y-DOTA-(Pro1,Tyr4)-bombesin(1-14). Bioconjug Chem.
9 Schuhmacher J., Zhang H., Doll J., Macke H.R., Matys R., Hauser H., Henze M., Haberkorn U., Eisenhut M. (2005). GRP receptor-targeted PET of a rat pancreas carcinoma xenograft in nude mice with a 68Ga-labeled bombesin(6-14) analog. J Nucl Med.
10 Hoffman T.J., Gali H., Smith C.J., Sieckman G.L., Hayes D.L., Owen N.K., Volkert W.A. (2003). Novel series of 111In-labeled bombesin analogs as potential radiopharmaceuticals for specific targeting of gastrin-releasing peptide receptors expressed on human prostate cancer cells. J Nucl Med.
11 Winkelmann, C.T., S.D. Figueroa, G.L. Sieckman, T.L. Rold, and T.J. Hoffman, Non-invasive MicroCT Imaging Characterization and In Vivo Targeting of BB2 Receptor Expression of a PC-3 Bone Metastasis Model. Mol Imaging Biol, 2012